# ^111^In-DPC11870

Chemical name: | ^111^In-DPC11870
Abbreviated name: | ^111^In-DPC11870
Synonym: | Divalent DTPA-conjugated LTB_4_ antagonist 17
Agent Category: | Compound
Target: | Leukotriene B_4_ receptor
Target Category: | Receptor
Method of detection: | Single photon emission computed tomography (SPECT); Planar gamma imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DPC11870)]]

The mobilization and activation of leukocytes during an inflammatory response is mediated through the binding of leukotriene B_4_ (LTB_4_) to its receptor on the membrane of these cells. On the basis of affinity, there are two known types of LTB_4_ receptors, BLT_1_ and BLT_2_ (1, 2). The BLT_1_ receptor is of the high-affinity type and is found primarily on neutrophils, and the BLT_2_ receptor is of the low-affinity variety that is found on most nucleated blood cells. Binding of LTB_4_ to the BLT receptors leads to chemotaxis and chemokinesis, which result in activation of granulocytes and macrophages as a response to inflammation and infection. Therefore, radiolabeled autologous leukocytes can be used for the detection and imaging of infection and inflammation. However, this in vitro process may require handling of contaminated blood, which puts the handler at risk for blood-borne infection. Investigators are in search of a radiochemical that would be convenient to handle and easy to prepare for the detection of infection and inflammation (3). In this regard, a variety of radiolabeled peptides and antibodies targeted toward specific receptors are now available for the diagnosis and imaging of infection and inflammation (4).

Because leukotrienes have an important role in the mediation of attraction and infiltration of granulocytes toward the sites of infection and inflammation, an LTB_4_ antagonist, ^111^indium (^111^In)-labeled DPC11870, has been investigated for potential scintigraphic imaging of these conditions (5). ^111^In-DPC11870 has been shown to bind to the BLT receptors on hematopoietic cells that accumulate at the site of infection in rabbits and could be used for imaging of the lesions (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In-DPC11870%20synthesis)]

The synthesis of ^111^In-DPC11870 has been detailed by van Eerd et al. (7). Briefly, ^111^In-DPC11870 synthesis was based on a polyethylene glycol derivative of SG385, another LTB_4_ antagonist (8). Blocked cysteic acid (boc-cysteic acid) and Glu(OTfp)-OTfp were prepared as described previously (9, 10). The tetra-cysteic acid derivative of SG385 was prepared by sequential addition of boc-cysteic acid in dimethylformamide to the benzotriazol-tetramethyluronium-hexafluorophosphate coupling reagent. The block was removed with a 50:50 trifluoroacetic acid:methylene chloride treatment and purification was performed by high-performance liquid chromatography (HPLC) on a C18 silica column after addition of the first, second, and fourth cysteic acids. The tetra-cysteic acid derivative product 11870 was recovered after HPLC by lyophilization and checked by HPLC and high-resolution mass spectroscopy. Dimerization of 11870 was achieved by a reaction of 11870 with bis-trifluoropropanone ester of blocked glutamic acid and hydroxyazabenzotriazole in dimethylformamide. The crude reaction product was treated with a combination of trifluoroacetic acid, methylene chloride, and triethylsilane to remove the remaining blocking group. The product was purified on a C18 column by HPLC. Conjugation with diethylenetriaminepentaacetic acid was performed by a reaction of diethylenetriaminepentaacetic acid anhydride in dimethylformamide. The final yield of unlabeled DPC11870 was 73% and HPLC analysis exhibited a single peak.

DPC11870 was labeled with ^111^In at pH 5.5 in ammonium acetate buffer for 30 min at room temperature. Radiochemical purity of the product as determined by instant thin-layer chromatography and reverse-phase HPLC was >99%, and the specific activity was 0.32 mCi/nmol (12 MBq/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In-DPC11870%20in%20vitro)]]

Using purified human granulocytes, the 50% inhibitory concentration (IC_50_) of ^111^In-DPC11870 was determined to be 10 nmol/L. In the presence of nonradioactive DPC11870, the radiochemical had high (40%) nonspecific binding but showed very low binding (<5%) to lymphocytes and erythrocytes (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In-DPC11870%20rodentia)]

To evaluate the use of ^111^In-DPC11870 for the visualization of infection in rabbits, the animals were given an intramuscular injection of Escherichia coli (3). Twenty-four hours later, when the infection was apparent by swelling, the rabbits were given an intravenous injection of ^111^In-DPC11870. Some animals received an injection of nonradioactive In-DPC11870 before the radiochemical was administered. This was done to saturate the LTB_4_ receptors for the determination of receptor-mediated accumulation of ^111^In-DPC11870. Radioactivity accumulated in the liver, lung, and kidney immediately after injection of the radiochemical and subsequently appeared in the spleen and bone marrow. Visualization of the abscess was observed two hours after injection and the visualization improved with time. Rabbits preinjected with the nonradioactive compound showed no appearance of the label at the site of the abscess, indicating that the abscess uptake of radioactivity was mediated by the receptor.

In another study (6), the abscess was visualized after rabbits were injected with the radiochemical and the E. coli infection was induced 16 h later. Another group of animals that showed signs of infection was administered heterologous leukocytes and bone marrow cells labeled in vitro with ^111^In-DPC11870. The biodistribution of ^111^In-DPC11870 was compared in the two groups of animals. An accumulation of radioactivity was observed at the site of the abscess in both groups of animals, confirming that the radioactivity accumulated at the site of infection because of the migration of the activated hematopoietic cells to the site of infection.

^111^In-DPC11870 was also shown to clearly visualize acute colitis lesions in rabbits less than one hour after injection of the radiolabel (11). The investigators also concluded that images acquired with ^111^In-DPC11870 were superior to those obtained with either ^99m^Tc-labeled granulocytes or fluorine [^18^F]FDG.

The use of ^111^In-DPC11870 to visualize experimentally induced pulmonary aspergillosis in rabbits was evaluated in comparison to ^67^Ga-citrate (7). Images were acquired 24 h after injection of the radiolabels, and the images obtained with ^111^In-DPC11870 were determined to be superior to the images obtained with ^67^Ga-citrate.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In-DPC11870%20Other%20Non-Primate%20Mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In-DPC11870%20Non-Human%20Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In-DPC11870%20Humans)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Yokomizo T., Izumi T., Chang K., Takuwa Y., Shimizu T. (1997). A G-protein-coupled receptor for leukotriene B4 that mediates chemotaxis. Nature.
2 Yokomizo T., Kato K., Terawaki K., Izumi T., Shimizu T. (2000). A second leukotriene B(4) receptor, BLT2. A new therapeutic target in inflammation and immunological disorders. J Exp Med.
3 van Eerd J.E., Oyen W.J., Harris T.D., Rennen H.J., Edwards D.S., Liu S., Ellars C.E., Corstens F.H., Boerman O.C. (2003). A bivalent leukotriene B(4) antagonist for scintigraphic imaging of infectious foci. J Nucl Med.
4 Signore A., Chianelli M., D'Alessandria C., Annovazzi A. (2006). Receptor targeting agents for imaging inflammation/infection: where are we now?. Q J Nucl Med Mol Imaging.
5 Broekema M., van Eerd J.J., Oyen W.J., Corstens F.H., Liskamp R.M., Boerman O.C., Harris T.D. (2005). Synthesis of leukotriene B4 antagonists labeled with In-111 or Tc-99m to image infectious and inflammatory foci. J Med Chem.
6 van Eerd J.E., Oyen W.J., Harris T.D., Rennen H.J., Edwards D.S., Corstens F.H., Boerman O.C. (2005). Scintigraphic imaging of infectious foci with an 111In-LTB4 antagonist is based on in vivo labeling of granulocytes. J Nucl Med.
7 van Eerd J.E., Rennen H.J., Oyen W.J., Harris T.D., Edwards D.S., Corstens F.H., Boerman O.C. (2004). Scintigraphic detection of pulmonary aspergillosis in rabbits with a radiolabeled leukotriene b4 antagonist. J Nucl Med.
8 Barrett, J.A., E.H. Cheesman, T.D. Harris, and M. Rajopadhye, Radiopharmaceuticals for imaging infection and inflammation., in PCT Int Appl WO 9815294. 1998, Bristol Meyer Squibb.
9 Harris, T.D., J.A. Barrett, A.P. Carpenter, and M. Rajopadhye, Vitronectin receptorantagonist pharmaceuticals., in US patent 6511649 2003, Bristol Meyer Squibb.
10 Hubbuch A., Danho W., Zahn H. (1979). Synthesis of N-protected cysteic acid derivatives and their activated derivatives. Liebigs Ann Chem.
11 van Eerd J.E., Laverman P., Oyen W.J., Harris T.D., Edwards D.S., Ellars C.E., Corstens F.H., Boerman O.C. (2004). Imaging of experimental colitis with a radiolabeled leukotriene B4 antagonist. J Nucl Med.